# 2-[^18^F]Fluoro-N-(2-(2-nitro-1H-imidazol-1-yl)ethyl)acetamide

Chemical name: | 2-[^18^F]Fluoro-N-(2-(2-nitro-1H-imidazol-1-yl)ethyl)acetatamide
Abbreviated name: | [^18^F]NEFA, [^18^F]7
Synonym:
Agent Category: | Compound
Target: | Hypoxic tissue
Target Category: | Hypoxia
Method of detection: | Positron emission tomography
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%202-Nitroimidazole)]

Hypoxia is found in a variety of solid tumors and leads to tumor progression and the resistance of tumors to chemotherapy and radiotherapy (1-3). Tumor oxygenation is heterogeneously distributed within human tumors (4). It would be beneficial to assess tumor oxygenation before and after therapy to provide an evaluation of tumor response to treatment and an insight into new therapeutic treatments (5). Tumor oxygenation is measured invasively using computerized, polarographic, oxygen-sensitive electrodes, which is regarded as the gold standard (6). Functional and non-invasive imaging of intratumoral hypoxia has been demonstrated to be feasible for the measurement of tumor oxygenation (7).

Chapman proposed the use of 2-nitroimidazoles for hypoxia imaging in 1979 (8). 2-Nitroimidazole compounds are postulated to undergo a reduction in hypoxic conditions, forming highly reactive oxygen radicals that subsequently bind covalently to macromolecules inside the cells (9). In normoxic conditions, the reduced molecule is rapidly reoxidized and transported from the cell. [^18^F]Fluoromisonidazole ([^18^F]FMISO (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=FMISO)) is the most widely used positron emission tomography tracer for imaging tumor hypoxia (7). However, it has slow clearance kinetics and high lipophilicity, resulting in substantial background signal in PET scans. [^18^F]Fluoroazomycinarabinofuranoside ([^18^F]FAZA (http://www.ncbi.nlm.nih.gov/books/NBK23282/)) is a 2-nitroimidazole with a sugar addition (10) and has been studied as a hypoxia-imaging agent, showing promising results in various tumor models in rats and mice (11, 12). Zha et al. (13) reported a new [^18^F]-labeled 2-nitroimidazole derivative, 2-[^18^F]fluoro-N-(2-(2-nitro-1H-imidazol-1-yl)ethyl)acetamide ([^18^F]NEFA), which contains a hydrolyzable amide group for in vivo hypoxic tissue imaging.

### Related Resource Links:

- Chapters in MICAD (Hypoxia (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Hypoxia+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Hypoxia-inducible factor 1, alpha subunit (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3091))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Hypoxia (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=hypoxia%5BAll+Fields%5D))
- Clinical trials (Hypoxia imaging (http://www.clinicaltrials.gov/ct2/results?term=hypoxia+imaging))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NEFT%20and%20synthesis)]

[^18^F]NEFA was readily synthesized by ^18^F-fluorination of 2-bromo-N-(2-(2-nitro-1H-imidazol-1-yl)ethyl)acetamide ([^18^F]KF/18-crown-6/KHCO_3_, 10 min at 90°C) in dimethyl sulfoxide (13). [^18^F]NEFA was purified with solid-phase extraction. Overall yield was 6%–7% at the end of synthesis, with a radiochemical purity of >98%. Total synthesis time was ~60 min. The specific activity of [^18^F]NEFA was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NEFT%20and%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NEFT%20and%20rodentia)]

Ex vivo biodistribution studies of [^18^F]NEFA were performed in mice (n = 3) bearing EMT-6 tumors at 30 min after injection (13). The tumor accumulation was 1.55 ± 0.65% injected dose/gram (ID/g). The liver (2.55% ID/g) had the highest accumulation, followed by the kidney (2.04% ID/g), lung (1.93% ID/g), bone (1.83% ID/g), heart (1.77% ID/g), blood (1.61% ID/g), spleen (1.59% ID/g), muscle (1.36% ID/g), and brain (0.99% ID/g). The tumor/blood, tumor/liver, and tumor/muscle ratios were 0.96, 0.61, and 1.14, respectively. These ratios for [^18^F]FMISO were 0.91, 0.59, and 1.74, respectively. The authors suggested that enzymatic or chemical hydrolysis of [^18^F]NEFA would yield [^18^F]fluoroacetate. It is difficult to determine if the hypoxia or the trapping of [^18^F]fluoroacetate or both is more important for tumor accumulation. No blocking study was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NEFT%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NEFT%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NEFT%20and%20humans)]

No publication is currently available.

## NIH Support

AG 022559-01

## References

1 Serkies K., Jassem J. (2005). Chemotherapy in the primary treatment of cervical carcinoma. Crit Rev Oncol Hematol.
2 Vaupel P., Mayer A. (2005). Hypoxia and anemia: effects on tumor biology and treatment resistance. Transfus Clin Biol.
3 Rajendran J.G., Krohn K.A. (2005). Imaging hypoxia and angiogenesis in tumors. Radiol Clin North Am.
4 Vaupel P., Harrison L. (2004). Tumor hypoxia: causative factors, compensatory mechanisms, and cellular response. Oncologist.
5 Dehdashti F., Grigsby P.W., Mintun M.A., Lewis J.S., Siegel B.A., Welch M.J. (2003). Assessing tumor hypoxia in cervical cancer by positron emission tomography with 60Cu-ATSM: relationship to therapeutic response-a preliminary report. Int J Radiat Oncol Biol Phys.
6 Raleigh J.A., Dewhirst M.W., Thrall D.E. (1996). Measuring Tumor Hypoxia. Semin Radiat Oncol.
7 Foo S.S., Abbott D.F., Lawrentschuk N., Scott A.M. (2004). Functional imaging of intratumoral hypoxia. Mol Imaging Biol.
8 Chapman J.D. (1979). Hypoxic sensitizers--implications for radiation therapy. N Engl J Med.
9 Chapman J.D., Baer K., Lee J. (1983). Characteristics of the metabolism-induced binding of misonidazole to hypoxic mammalian cells. Cancer Res.
10 Reischl G., Ehrlichmann W., Bieg C., Solbach C., Kumar P., Wiebe L.I., Machulla H.J. (2005). Preparation of the hypoxia imaging PET tracer [18F]FAZA: reaction parameters and automation. Appl Radiat Isot.
11 Piert M., Machulla H.J., Picchio M., Reischl G., Ziegler S., Kumar P., Wester H.J., Beck R., McEwan A.J., Wiebe L.I., Schwaiger M. (2005). Hypoxia-specific tumor imaging with 18F-fluoroazomycin arabinoside. J Nucl Med.
12 Sorger D., Patt M., Kumar P., Wiebe L.I., Barthel H., Seese A., Dannenberg C., Tannapfel A., Kluge R., Sabri O. (2003). [18F]Fluoroazomycinarabinofuranoside (18FAZA) and [18F]Fluoromisonidazole (18FMISO): a comparative study of their selective uptake in hypoxic cells and PET imaging in experimental rat tumors. Nucl Med Biol.
13 Zha Z., Zhu L., Liu Y., Du F., Gan H., Qiao J., Kung H.F. (2011). Synthesis and evaluation of two novel 2-nitroimidazole derivatives as potential PET radioligands for tumor imaging. Nucl Med Biol.